# ^99m^Tc-Tricarbonyl-His_6_-annexin A5

Chemical name: | ^99m^Tc-Tricarbonyl-His_6_-annexin A5
Abbreviated name: | ^99m^Tc(CO)_3_-His-A5
Synonym:
Agent category: | Protein
Target: | Phosphatidylserine (PS)
Target category: | Phospholipid
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal\contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=468888), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=4809273) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=308) for more information about annexin V.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Annexin%20A5%20and%2099mTc)]

Apoptosis (programmed cell death) plays an important role in the pathophysiology of many diseases, such as cancers, neurodegenerative disorders, vascular disorders, atherosclerosis, and chronic hepatitis, as well as in the biology of normal cells like epithelial cells and immune cells (1). During apoptosis, there is rapid redistribution of phosphatidylserine (PS) from the inner membrane leaflet to the outer membrane leaflet, exposing the anionic head group of PS. PS is also accessible for annexin V (or annexin A5) binding in necrosis because of disruption of the plasma membrane. Annexin V, a 36-kDa protein, binds to PS with high affinity (K_d_ = 7 nM). Annexin V derivatives have been developed for imaging apoptosis as well as necrosis with different imaging modalities such as single-photon emission computed tomography (SPECT) (2-4), positron emission tomography (5), near-infrared (NIR) fluorescence (6), and magnetic resonance imaging (7). His_6_-Tagged annexin A5 was radiolabeled with ^99m^Tc using tricarbonyl chemistry (^99m^Tc(CO)_3_-His-A5) for noninvasive in vivo SPECT imaging of apoptosis in mice (8, 9).

### Related Resource Links:

- Chapters in MICAD (Annexin V (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=Annexin%20V+AND+micad%5Bbook%5D))
- Gene information in NCBI (Annexin V (http://www.ncbi.nlm.nih.gov/gene/308))
- Articles in Online Mendelian Inheritance in Man (OMIM) (Annexin V (http://www.ncbi.nlm.nih.gov/omim/131230))
- Clinical trials (Annexin V (http://www.clinicaltrials.gov/ct2/results?term=Annexin+V+))
- Drug information in FDA (Annexin V (http://google2.fda.gov/search?q=annexin+V&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=3&y=8))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Annexin%20A5%2099mTc%20and%20synthesis)]

A solution of [^99m^Tc(H_2_O)_3_(CO)_3_]^+^ and His_6_-tagged annexin A5 was incubated for 90 min at 37°C (8). ^99m^Tc(CO)_3_-His-A5 was isolated with column chromatography with radiochemical purity of >95% and radiochemical yields of 70%–85%. The specific activities were 192–220 MBq/nmol (5.2–6.0 mCi/nmol). ^99m^Tc(CO)_3_-His-A5 was stable for up to 24 h at 4°C and 37°C in saline and cell culture medium with 10% fetal bovine serum. ^99m^Tc(CO)_3_-His-A5 was also stable in in human serum for up to 4 h at 37°C.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Annexin%20A5%2099mTc%20and%20in%20vitro)]

Vangestel et al. (8) performed cell-binding assays with ^99m^Tc(CO)_3_-His-A5 in human Colo205 colon cancer cells in the absence and presence of 1 mM 5-fluorouracil (5-FU) to induce apoptosis at 4 h and 24 h after incubation. The 5-FU-treated cells exhibited 38% and 106% increases in radioactivity (P < 0.05) at 4 h and 24 h, respectively compared with untreated cells at the same time points. The 5-FU-treated cells incubated with annexin A5-FITC showed 24% apoptotic cells at 24 h, whereas only 4% apoptotic cells were shown in the untreated cells (P < 0.05).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Annexin%20A5%2099mTc%20and%20rodentia)]

Vangestel et al. (8) performed SPECT imaging studies in nude mice (n = 5) for the first 100 min and then at 4, 8, and 22 h after injection of 37 MBq (1 mCi) ^99m^Tc(CO)_3_-His-A5. The blood levels were 7% injected dose/gram (ID/g) and 1% ID/g at 10 min and 100 min after injection. The kidneys exhibited the highest radioactivity at all the time points of the studies, with the maximum level (29% ID/g) at 40 min after injection. The initial accumulation in the liver was 13% ID/g at 10 min and declined to 9% at 100 min. Low radioactivity was observed in the thyroid and stomach, suggesting the absence of ^99m^Tc-pertechnetate in the circulation.

In another experiment, imaging studies were performed in nude mice (n = 12) bearing Colo205 tumors to measure spontaneous tumor apoptosis at 3.5 h after injection of ^99m^Tc(CO)_3_-His-A5. The tumor radioactivity levels ranged from 0.15%–0.35% ID/g. Ex vivo immunohistochemical analysis of the tumor sections showed 1.4 ± 0.4% apoptotic (caspase-3-positive) cells in the tumors and correlated well with ^99m^Tc(CO)_3_-His-A5 accumulation (R = 0.867, P < 0.01). No blocking and ex vivo biodistribution studies were performed.

Vangestel et al. (9) performed SPECT imaging studies in nude mice (n = 3/group) bearing Colo205 tumors to measure tumor apoptosis after treatments with buffer, 5-FU (250 mg/kg), irinotecan (100 mg/kg), oxaliplatin (30 mg/kg), anti-VEGF bevacizumab (5 mg/kg), and anti-EGFR panitumumab (6 mg/kg) at 4, 8, 12, 24, and 48 h after injection of ^99m^Tc(CO)_3_-His-A5. Bevacizumab-treated mice showed no increase in accumulation of ^99m^Tc(CO)_3_-His-A5, and a peak of ^99m^Tc(CO)_3_-His-A5 uptake in panitumumab-treated mice was observed at 24 h after injection, as confirmed with caspase-3 immunostaining. For irinotecan-, oxaliplatin-, and bevacizumab-treated tumors, a significant correlation was observed between the ^99m^Tc(CO)_3_-His-A5 accumulation and caspase-3 immunostaining (r = 0.8, P < 0.05; r = 0.9, P < 0.001; r = 0.9, P < 0.001, respectively). For 5-FU- and panitumumab-treated mice, the correlation coefficients were not significant (r = 0.7, P = 0.18; r = 0.7, P = 0.19, respectively).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Annexin%20A5%2099mTc%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Annexin%20A5%2099mTc%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Annexin%20A5%2099mTc%20and%20human)]

No publication is currently available.

## References

1 Thompson C.B. (1995). Apoptosis in the pathogenesis and treatment of disease. Science.
2 Blankenberg F.G. (2004). Recent advances in the imaging of programmed cell death. Curr Pharm Des.
3 Keen H.G., Dekker B.A., Disley L., Hastings D., Lyons S., Reader A.J., Ottewell P., Watson A., Zweit J. (2005). Imaging apoptosis in vivo using 124I-annexin V and PET. Nucl Med Biol.
4 Lahorte C., Slegers G., Philippe J., Van de Wiele C., Dierckx R.A. (2001). Synthesis and in vitro evaluation of 123I-labelled human recombinant annexin V. Biomol Eng.
5 Murakami Y., Takamatsu H., Taki J., Tatsumi M., Noda A., Ichise R., Tait J.F., Nishimura S. (2004). 18F-labelled annexin V: a PET tracer for apoptosis imaging. Eur J Nucl Med Mol Imaging.
6 Schellenberger E.A., Sosnovik D., Weissleder R., Josephson L. (2004). Magneto/optical annexin V, a multimodal protein. Bioconjug Chem.
7 van Tilborg G.A., Mulder W.J., Deckers N., Storm G., Reutelingsperger C.P., Strijkers G.J., Nicolay K. (2006). Annexin A5-functionalized bimodal lipid-based contrast agents for the detection of apoptosis. Bioconjug Chem.
8 Vangestel C., Peeters M., Oltenfreiter R., D'Asseler Y., Staelens S., Van Steenkiste M., Philippe J., Kusters D., Reutelingsperger C., Van Damme N., Van de Wiele C. (2010). In vitro and in vivo evaluation of [99mTc]-labeled tricarbonyl His-annexin A5 as an imaging agent for the detection of phosphatidylserine-expressing cells. Nucl Med Biol.
9 Vangestel C., Van de Wiele C., Mees G., Mertens K., Staelens S., Reutelingsperger C., Pauwels P., Van Damme N., Peeters M. (2012). Single-Photon Emission Computed Tomographic Imaging of the Early Time Course of Therapy-Induced Cell Death Using Technetium 99m Tricarbonyl His-annexin A5 in a Colorectal Cancer Xenograft Model. Mol Imaging.